# MICAD supplemental information disclaimer

The MICAD supplemental information section contains unpublished information submitted by members of the imaging community on a voluntary basis. The information is presented "as is", and it has not been reviewed by the MICAD staff for its accuracy, reliability, completeness, currency, legality, quality, or appropriateness. The supplemental information is subject to the same copyright and disclaimers as the rest of the MICAD content:

1. Please read carefully our complete disclaimer (http://www.ncbi.nlm.nih.gov/About/disclaimer.html) information before submitting supplemental information for inclusion into MICAD.
2. The supplemental information should be related to the specific agent and will give additional relevant information not already summarized in the MICAD chapter.